# Radioiodinated (Z)-2-(4-(2-hydroxyethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one

Chemical name: | Radioiodinated (Z)-2-(4-(2-hydroxyethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one | [image]
Abbreviated name: | [^125^I]15 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Humans | Structures of aurone derivatives by Maya et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

Radioiodinated (Z)-2-(4-(2-hydroxyethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one (compound 15), abbreviated as [^125^I]15, is an aurone derivative synthesized by Maya et al. for single-photon emission computed tomography(SPECT) of Alzheimer’s disease (AD) by targeting β-amyloid (Aβ) (1). The other four aurone derivatives include radioiodinated (Z)-2-(4-methoxybenzylidene)-5-iodobenzofuran-3(2H)-one (compound 9), (Z)-2-(4-hydroxybenzylidene)-5-iodobenzofuran-3(2H)-one (compound 14), (Z)-2-(4-(2-(2-hydroxyethoxy)ethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one (compound 16), and (Z)-2-(4-(2-(2-(2-hydroxyethoxy)ethoxy)ethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one (compound 17), which are abbreviated as [^125^I]9, [^125^I]14, [^125^I]16, and [^125^I]17, respectively.

AD is characterized in pathology by the presence of extracellular Aβ plaques, intraneuronal neurofibrillary tangles, and neuronal loss in the cerebral cortex (2, 3). Of them, Aβ deposit is the earliest neuropathological marker and is relatively specific to AD and closely related disorders. Aβ plaques are composed of abnormal paired helical filaments 5–10 nm in size. These filaments are largely made of insoluble Aβ peptides that are 40 or 42 amino acids in length (4).

In recent years, molecular imaging by targeting the extracellular Aβ has been intensively investigated in attempts to detect early AD, assess Aβ content in vivo, determine the timing of anti-plaque therapy, and evaluate the therapeutic efficacy (4). Radiolabeled Aβ40 peptides were tested first, but they showed poor penetration ability to cross the blood–brain barrier (BBB) (4). Based on the fact that Aβ can be specifically stained in vitro with dyes of Congo red, chrysamine G, and thioflavin-T, an effort was made to develop imaging agents with these dyes. This effort, however, was in general unsuccessful because the bulky ionic groups of heteroatoms in these dyes prevent them from crossing the BBB (2). Importantly, a large class of derivatives (e.g., aminonaphthalenes, benzothiazoles, stilbenes, and imidazopyridines) was synthesized with these dyes as templates (4). Clinical and preclinical studies have shown that these derivatives not only possess a high binding affinity with Aβ plaques as their parent compounds, but also exhibit good penetration ability through the BBB and rapid washout from brain with low to no plaque deposits.

Ono et al. first synthesized a class of radioiodinated flavone derivatives that present a high binding affinity with Aβ plaques and good penetration ability through the BBB (5). However, these flavone derivatives display poor clearance from the brain, which leads to a high brain background. The investigators then explored another class of flavonoids with aurone as the core structure (6, 7). Aurone is a heterocyclic chemical compound that contains a benzofuran element associated with a benzylidene linked in position 2 and a chalcone-like group being closed into a five-member ring. The aurone derivatives possess a nucleophilic group (NH_2_, NHMe, or NMe_2_) at the 4' position and a radioiodine at the 5 position. Although these aurone derivatives exhibit a strong binding affinity with Aβ (inhibition constant (K_i_) = 1.2–6.8 nM), high penetration ability through the BBB (1.9%−4.6% injected dose per gram tissue (ID/g) at 2 min), and a fast washout from the brain (0.3%−0.5% ID/g at 30 min), the pharmacokinetics of these compounds are less favorable for brain imaging than the pharmacokinetics of the agent [^123^I]IMPY (6-iodo-2-(4'-dimethylamino)phenyl-imidazo[1,2]pyridine), which is the only SPECT agent to be tested in humans to date (1, 8, 9). The investigators also modified the flavone and aurone derivatives by pegylating them with 1–3 units of ethylene glycol at the 4' position or by conjugating them with the chelating agent bis-amino-bis-thiol (BAT) (7). Favorable pharmacokinetics for brain imaging was observed for the pegylated derivatives ([^18^F]8(a–c)) but not for the BAT-chelated derivatives ([^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR) (6, 7).

This series of chapters summarizes the data obtained with flavone and aurone derivatives, including [^125^I]15, [^125^I]9, [^125^I]14, [^125^I]16, [^125^I]17, [^99m^Tc]BAT-FL, [^99m^Tc]BAT-AR, [^18^F]8(a–c), [^125^I]3, and [^18^F]3 (1, 6-8). This chapter presents the data obtained with [^125^I]15, [^125^I]9, [^125^I]14, [^125^I]16, and [^125^I]17 (1).

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ono%20and%20maya)]

The aurone backbone was synthesized by an Aldol reaction of benzofuranones with benzaldehydes using Al_2_O_3_ in chloroform at room temperature (1). The tributyltin derivatives were prepared by using a halogen-to-tributyltin exchange reaction catalyzed by Pd(0). Radioiodination of the tributyltin derivatives resulted in the agents [^125^I]9, [^125^I]14, [^125^I]15, [^125^I]16, and [^125^I]17. The radiochemical identities of the radioiodinated compounds were verified by coinjection with nonradioactive compounds with high-performance liquid chromatography (HPLC). The radiochemical yields were 25%−57%, and the radiochemical purities were >95% after purification with HPLC. It was anticipated that the no-carrier-added preparation would result in a final product bearing a theoretical specific activity similar to that of ^125^I (81.4 TBq/mmol (2,200 Ci/mmol)).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19072219)]

The binding affinities of the unradiolabeled compounds 9, 14, 15, 16, and 17 were measured with Aβ(1−42) aggregates using (Z)-2-(4-aminobenzylidene)-5-iodobenzofuran-3(2H)-one ([^125^I]AAU, K_d_ = 4.2 nM) as the competing radioligand (5). The K_i_ values estimated for compounds 9, 14, 15, 16, and 17 were 2.9, 1.3, 1.1, 3.4, and 2.6 nM, respectively, similar to the values of known Aβ imaging agents such as SB-13 (1.2 nM), PIB (2.8 nM), and IMPY (1.4 nM), indicating that these aurone derivatives have binding affinity strong enough to test clinically (1).

The binding of the aurone derivatives with mouse Aβ plaques was confirmed in brain sections of double transgenic AD mice (Tg2576) (1). Fluorescent staining showed that many amyloid plaques were clearly stained with the derivatives, and the labeling patterns were consistent with that observed with thioflavin S staining. These results suggest that these aurone derivatives can specifically bind with Aβ plaques in the mouse brain.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19072219)]

Biodistribution studies were performed in normal ddY mice (n = 4–5 mice/time point for each agent) after tail vein injection of the agents (4.2−6.3 kBq (113.5–170.3 nCi)) (1). The brain uptake values ranged from 1.7% to 4.5% ID/g (4.51% ID/g for [^125^I]15) at 2 min after injection, a level sufficient for imaging Aβ plaques in the brain. The five agents also displayed good clearance from the normal brain (0.1%−0.4% ID/g (0.24% ID/g for [^125^I]15) at 30 min after injection). The brain_2min_/brain_30min_ ratios (an index of the washout rate) for [^125^I]9, [^125^I]14, [^125^I]15, [^125^I]16, and [^125^I]17 were 15.4, 8.3, 18.8, 9.7, and 15.6, respectively. [^125^I]15 had the best washout index and was superior to [^123^I]IMPY (11.1). The kidney, liver, and intestine were the normal organs with the highest radioactivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19072219)]

Postmortem brain tissues from an autopsy-confirmed case of AD and a control subject were used to analyze the binding of [^125^I]15 with human Aβ plaques in brain sections with autoradiography (1). High radioactivity was observed in the brain sections, and the hot spots were consistent with those observed with in vitro immunohistochemical staining in the same brain sections. Normal human brain displayed no evident accumulation of [^125^I]15. These results demonstrate the feasibility of using [^125^I]15 as a SPECT probe for detecting Aβ plaques in the brains of AD patients.

## References

1 Maya Y., Ono M., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). Novel radioiodinated aurones as probes for SPECT imaging of beta-amyloid plaques in the brain. Bioconjug Chem.
2 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
3 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Ono M., Maya Y., Haratake M., Ito K., Mori H., Nakayama M. (2007). Aurones serve as probes of beta-amyloid plaques in Alzheimer's disease. Biochem Biophys Res Commun.
6 Ono M., Watanabe R., Kawashima H., Kawai T., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). 18F-labeled flavones for in vivo imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem.
7 Ono M., Ikeoka R., Watanabe H., Kimura H., Fuchigami T., Haratake M., Saji H., Nakayama M. (2010). 99mTc/Re complexes based on flavone and aurone as SPECT probes for imaging cerebral beta-amyloid plaques. Bioorg Med Chem Lett.
8 Watanabe H., Ono M., Kimura H., Kagawa S., Nishii R., Fuchigami T., Haratake M., Nakayama M., Saji H. (2011). A dual fluorinated and iodinated radiotracer for PET and SPECT imaging of beta-amyloid plaques in the brain. Bioorg Med Chem Lett.
9 Newberg A.B., Wintering N.A., Plossl K., Hochold J., Stabin M.G., Watson M., Skovronsky D., Clark C.M., Kung M.P., Kung H.F. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.